# ^68^Ga-Labeled (1,4,7,10-tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid)-1-NaI3-octreotide

Chemical name: | ^68^Ga-Labeled (1,4,7,10-tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid)-1-NaI3-octreotide
Abbreviated name: | [^68^Ga]-DOTA-NOC
Synonym:
Agent Category: | Ligand
Target: | Somatostatin receptors 2, 3 and 5 (sstr2, sstr3 and sstr5)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+DOTA-NOC)]

Neuroendocrine tumors (NTs) are slow growing, can develop in almost any organ of the body (1), and are characterized by the overexpression of somatostatin receptors (sstr; designated 1–5) (2). Because the different sstrs may be expressed individually or simultaneously by the NT, these receptors are targeted with radiolabeled compounds for the imaging detection or the treatment of this ailment (3). Due to a very short plasma half-life (~3 min), somatostatin itself is not the preferred sstr ligand for radiolabeling, and several of its analogs, such as octreotide (OC), vapreotide, etc., have been developed for the imaging and therapy of NTs (4). OCs show a high affinity for sstr2 and sstr5, but they bind varyingly to the sstr3 and sstr4 receptors. The OCs are coupled with chelators like diethylenetriamine-pentaacetic acid (DTPA) or 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) to facilitate nuclide binding before use with scintigraphic imaging (with ^111^In or ^99m^Tc (5, 6)) or positron emission tomography (PET; with ^18^F, ^64^Cu, or ^68^Ga (7-9)) of NTs. The main advantage of using PET over planar scintigraphy is that the PET ligands do not have to be internalized by the cells to obtain good quality images of the NTs (10, 11).

Although (^18^F)fluoro-deoxyglucose has been used to detect tumors of neuroendocrine origin, it has been shown to have little success because it cannot detect well-differentiated NTs (12). As an alternative, (^111^In)DOTA-(tyrosine)^3^-octreotide ((^111^In)DOTA-TOC) was developed to detect NTs, but it too has limited application because it binds only to the sstr2 receptors and cannot detect NETs that express the other sstr subtypes (3). To circumvent this limitation, investigators developed (13) and evaluated (14) a ^68^Ga-labeled sstr ligand, DOTA-1-NaI3-octreotide ((^68^Ga)-DOTA-NOC), that binds sstr2, sstr3, and sstr5 (13). This was generated by substituting the third Phe moiety in OC (D-Phe-C[Cys-Phe-D-Trp-Lys-Thr-Cys]-Thr-ol) with napthyl-L-Ala (15). The biodistribution of (^68^Ga)-DOTA-NOC in humans has also been reported (16).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga-DOTA-NOC+synthesis)]

DOTA-NOC used for the various studies was either synthesized as described by Wild et al. (13) or obtained from a commercial source (9). The ^68^Ga labeling of DOTA-NOC was performed as described by Meyer et al. (17). In another publication describing the radiolabeling of DOTA-NOC with ^68^Ga, the radiochemical yield and purity of the radiochemical were reported to be 81.6 ± 6.5% and >99%, respectively (15). The specific activity and stability of (^68^Ga)-DOTA-NOC were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga-DOTA-NOC+in+vitro)]

The receptor binding characteristics of ^111^In-labeled DOTA-NOC were studied by Wild et al. (13) under in vitro conditions using cell lines respectively transfected with the various human sstr (hsstr) receptors as detailed by Reubi et al. (18). The 50% inhibition concentrations (in nM) of (^111^In)-DOTA-NOC for hsstr1, hsstr2, hsstr3, hsstr4, and hsstr5 were reported to be >1,000, 3.3 ± 0.2, 26 ± 1.9, >1,000, and 10.4 ± 1.6, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga-DOTA-NOC+rodentia)]

No references are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga-DOTA-NOC+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga-DOTA-NOC+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

In a preliminary study, the uptake of (^111^In)-DOTA-TOC (using planar imaging) and (^68^Ga)-DOTA-NOC (using PET imaging) in a 52-year-old patient with advanced neuroendocrine tumors was compared by Wild et al. (14). The investigators reported that bone metastasis in the patient was more clearly visible with (^68^Ga)-DOTA-NOC than with (^111^In)-DOTA-TOC. In addition, compared with (^111^In)-DOTA-TOC, superior images of organs that are known to express the different sstr rather than just sstr2 (such as spleen, pituitary, and thyroid), were obtained with (^68^Ga)-DOTA-NOC. From this preliminary study the investigators concluded that (^68^Ga)-DOTA-NOC could be an excellent radiodiagnostic and investigational chemical for sstr-positive tumors.

Pettinato et al. investigated the biodistribution of (^68^Ga)-DOTA-NOC in patients with neuroendocrine tumors (16). Nine patients were treated with (^68^Ga)-DOTA-NOC, and whole-body PET scans were performed at 5, 20, 60, and 120 min after administration of the radiochemical. Urine samples were also collected from the patients at approximately the same time as the scans, and blood samples were obtained every 40 to 50 min after treatment with (^68^Ga)-DOTA-NOC. In all patients an accumulation of the radiochemical was observed in the pituitary gland, spleen, liver, kidneys, and urinary bladder. The kidneys had the highest absorbed dose, probably because the radioactivity was excreted primarily through the urinary route.

Ambrosini et al. compared the use of (^18^F)3,4-dihydroxy-L-phenylalanine ((^18^F)-DOPA) with the use of (^68^Ga)-DOTA-NOC for the detection of gastro-entero-pancreatic and lung neuroendocrine tumors in 13 patients (19). PET imaging with (^68^Ga)-DOTA-NOC was reported to show at least one lesion in each of the 13 patients, but (^18^F)-DOPA visualized positive lesions in only 9 of the 13 patients. In addition, (^68^Ga)-DOTA-NOC identified more lesions than did (^18^F)-DOPA (71 versus 45), particularly in the liver, lungs, and lymph nodes. In addition, (^68^Ga)-DOTA-NOC correctly identified the primary site of the tumors in six of the eight non-operated cases, whereas (^18^F)-DOPA identified the primary tumors only in two of the eight non-operated cases. The investigators concluded that (^68^Ga)-DOTA-NOC appeared to be a superior imaging agent for the detection of neuroendocrine tumors compared with (^18^F)-DOPA.

Fanti et al. evaluated the use of (^68^Ga)-DOTA-NOC for the detection of unusual neuroendocrine tumors in 14 patients (13 patients had lesions that were either uterine or located in the prostate, ovary, kidney, breast, ear, neck, abdomen, or mediastinum, and one patient had a lymphoma) (10). Results obtained with PET imaging were compared with those obtained with computed tomography (CT), ultrasonography, magnetic resonance, and SSR scintigraphy. PET imaging identified at least one lesion in 6 of 14 patients; five scans were negative and two were inconclusive. At the clinical level, (^68^Ga)-DOTA-NOC, in comparison to the conventional imaging procedures, provided additional information in 7 of 14 patients and was considered helpful for 12 of 14 patients. With results from this study, the investigators concluded that (^68^Ga)-DOTA-NOC could be used to detect unusual neuroendocrine tumors particularly in the neck, abdomen, and mediastinum, but cautioned that care was required to investigate lesions in an organ having a high accumulation of the radioactivity or if inflammation was evident at the lesion site.

Ambrosini et al. evaluated the use of (^68^Ga)-DOTA-NOC with PET/CT for the identification of well-differentiated and proven bronchial carcinoids in 11 patients (9). The PET results were compared with pathology, clinical investigations, and contrast-enhanced CT data. At least one lesion was detected in 9 of 11 patients, and two scans were negative according to (^68^Ga)-DOTA-NOC PET/CT. The PET/CT results did not agree with contrast-enhanced CT in 8 of 11 patients, and in 3 patients both techniques provided similar results. During the clinical investigation, PET/CT provided additional data for 9 of 11 patients and resulted in changes in the clinical management of 3 of 9 patients. The investigators concluded that using (^68^Ga)-DOTA-NOC with PET/CT was better than using contrast-enhanced CT alone for the evaluation and determination of the extent of the disease in patients with bronchial carcinoids.

## Supplemental Information

[Disclaimers]

## References

1 Insabato L., Del Basso De Caro M., Caramanna E., De Rosa G. (2009). Pathology of neuroendocrine tumours. Front Biosci.
2 Mankoff D.A., Link J.M., Linden H.M., Sundararajan L., Krohn K.A. (2008). Tumor receptor imaging. J Nucl Med.
3 Reubi J.C., Waser B. (2003). Concomitant expression of several peptide receptors in neuroendocrine tumours: molecular basis for in vivo multireceptor tumour targeting. Eur J Nucl Med Mol Imaging.
4 Koopmans, K.P., O.N. Neels, I.P. Kema, P.H. Elsinga, T.P. Links, E.G. de Vries, and P.L. Jager, Molecular imaging in neuroendocrine tumors: Molecular uptake mechanisms and clinical results. Crit Rev Oncol Hematol, 2009
5 Wang F., Wang Z., Wu J., Qu W., Yao W., Zhao J., Liu Z. (2008). The role of technetium-99m-labeled octreotide acetate scintigraphy in suspected breast cancer and correlates with expression of SSTR. Nucl Med Biol.
6 Suchak A.A., Millo N., MacEwan R., McEwan A.J. (2009). Neuroendocrine differentiated breast carcinoma with pleural metastases using indium-111 octreotide. Clin Nucl Med.
7 Anderson C.J., Dehdashti F., Cutler P.D., Schwarz S.W., Laforest R., Bass L.A., Lewis J.S., McCarthy D.W. (2001). 64Cu-TETA-octreotide as a PET imaging agent for patients with neuroendocrine tumors. J Nucl Med.
8 Meisetschlager G., Poethko T., Stahl A., Wolf I., Scheidhauer K., Schottelius M., Herz M., Wester H.J., Schwaiger M. (2006). Gluc-Lys([18F]FP)-TOCA PET in patients with SSTR-positive tumors: biodistribution and diagnostic evaluation compared with [111In]DTPA-octreotide. J Nucl Med.
9 Ambrosini V., Castellucci P., Rubello D., Nanni C., Musto A., Allegri V., Montini G.C., Mattioli S., Grassetto G., Al-Nahhas A., Franchi R., Fanti S. (2009). 68Ga-DOTA-NOC: a new PET tracer for evaluating patients with bronchial carcinoid. Nucl Med Commun.
10 Fanti S., Ambrosini V., Tomassetti P., Castellucci P., Montini G., Allegri V., Grassetto G., Rubello D., Nanni C., Franchi R. (2008). Evaluation of unusual neuroendocrine tumours by means of 68Ga-DOTA-NOC PET. Biomed Pharmacother.
11 Gabriel M., Decristoforo C., Kendler D., Dobrozemsky G., Heute D., Uprimny C., Kovacs P., Von Guggenberg E., Bale R., Virgolini I.J. (2007). 68Ga-DOTA-Tyr3-octreotide PET in neuroendocrine tumors: comparison with somatostatin receptor scintigraphy and CT. J Nucl Med.
12 Junik R., Drobik P., Malkowski B., Kobus-Blachnio K. (2006). The role of positron emission tomography (PET) in diagnostics of gastroenteropancreatic neuroendocrine tumours (GEP NET). Adv Med Sci.
13 Wild D., Schmitt J.S., Ginj M., Macke H.R., Bernard B.F., Krenning E., De Jong M., Wenger S., Reubi J.C. (2003). DOTA-NOC, a high-affinity ligand of somatostatin receptor subtypes 2, 3 and 5 for labelling with various radiometals. Eur J Nucl Med Mol Imaging.
14 Wild D., Macke H.R., Waser B., Reubi J.C., Ginj M., Rasch H., Muller-Brand J., Hofmann M. (2005). 68Ga-DOTANOC: a first compound for PET imaging with high affinity for somatostatin receptor subtypes 2 and 5. Eur J Nucl Med Mol Imaging.
15 Di Pierro D., Rizzello A., Cicoria G., Lodi F., Marengo M., Pancaldi D., Trespidi S., Boschi S. (2008). Radiolabelling, quality control and radiochemical purity assessment of the Octreotide analogue 68Ga DOTA NOC. Appl Radiat Isot.
16 Pettinato C., Sarnelli A., Di Donna M., Civollani S., Nanni C., Montini G., Di Pierro D., Ferrari M., Marengo M., Bergamini C. (2008). 68Ga-DOTANOC: biodistribution and dosimetry in patients affected by neuroendocrine tumors. Eur J Nucl Med Mol Imaging.
17 Meyer G.J., Macke H., Schuhmacher J., Knapp W.H., Hofmann M. (2004). 68Ga-labelled DOTA-derivatised peptide ligands. Eur J Nucl Med Mol Imaging.
18 Reubi J.C., Schar J.C., Waser B., Wenger S., Heppeler A., Schmitt J.S., Macke H.R. (2000). Affinity profiles for human somatostatin receptor subtypes SST1-SST5 of somatostatin radiotracers selected for scintigraphic and radiotherapeutic use. Eur J Nucl Med.
19 Ambrosini V., Tomassetti P., Castellucci P., Campana D., Montini G., Rubello D., Nanni C., Rizzello A., Franchi R., Fanti S. (2008). Comparison between 68Ga-DOTA-NOC and 18F-DOPA PET for the detection of gastro-entero-pancreatic and lung neuro-endocrine tumours. Eur J Nucl Med Mol Imaging.